# 2-(3,4-Dimethoxyphenyl)-5-[2-(3,4-dimethoxyphenyl)ethyl-[^11^C]methyl-amino]-2-propan-2-yl-pentanenitrile

Chemical name: | 2-(3,4-Dimethoxyphenyl)-5-[2-(3,4-dimethoxyphenyl)ethyl-[^11^C]methyl-amino]-2-propan-2-yl-pentanenitrile
Abbreviated name: | [^11^C]Verapamil
Synonym:
Agent category: | Compound
Target: | P-glycoprotein multidrug transporter, MDR-1
Target category: | Transporter
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-Human Primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%5BAll%20Fields%5D%20AND%20%28%22verapamil%22%5BMeSH%20Terms%5D%20OR%20Verapamil%5BText%20Word%5D%29)]

One of the mechanisms by which cells mitigate the cytotoxic effects of chemotherapeutic agents, such as Adriamycin, Vinca alkaloids, epipodophyllotoxins, actinomycin D, and Paclitaxel, is to limit their presence inside the cells via the transmembrane protein P-glycoprotein (P-gp), which is encoded by the multidrug resistance (MDR-1) gene (1, 2). P-gp is an ATP-dependent multidrug transporter that is capable of actively pumping a variety of agents out of cells. Injection of unlabeled efflux pump substrates increases retention of radioactivity in the tumor rather than lessen the radioactivity, as seen with receptor-binding radiotracers. Overexpression of P-gp in tumor cells (such as renal carcinoma, hepatoma, pheochromocytoma, and colon carcinoma) leads to resistance to anticancer drugs (3). P-gp is also present in a variety of normal cells, such as intestinal mucosal cells, hepatocytes, renal proximal tubule epithelial cells, and endothelial cells of the blood-brain barrier (BBB) (4). Calcium channel blockers, cyclosporin A, and its non-immunosuppressive analog PSC 833 are MDR modulators, inhibiting transport of P-gp substrates out of the cells (5, 6).

Sestamibi (MIBI) is a substrate for P-gp, ^99m^Tc-MIBI (http://www.ncbi.nlm.nih.gov/books/bv.fcgi?rid=micad.chapter.MIBI99mtc) has been approved by the U.S. Food and Drug Administration as a myocardial perfusion imaging agent with single-photon emission computed tomography (SPECT) to assess the risk of future cardiac events. It is also used as a tumor-imaging agent in breast, lung, thyroid, and brain cancers. Verapamil, a calcium channel blocker, is also a transport substrate for the P-gp efflux pump (7). [^11^C]Verapamil is being developed as a positron emission tomography (PET) agent for studying P-gp function non-invasively.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=P-glycoprotein%5BAll+Fields%5D+AND+micad%5Bbook%5D) (P-glycoprotein (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=P-glycoprotein%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (P-glycoprotein (http://www.ncbi.nlm.nih.gov/gene/5243))
- Articles in OMIM (P-glycoprotein (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=P-glycoprotein%5BAll+Fields%5D))
- Clinical trials (P-glycoprotein (http://www.clinicaltrials.gov/ct2/results?term=P-glycoprotein), Verapamil (http://www.clinicaltrials.gov/ct2/results?term=Verapamil))
- Drug information in FDA (^99m^Tc-MIBI (http://google2.fda.gov/search?q=99mTc-sestamibi+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=16), Verapamil (http://google2.fda.gov/search?q=verapamil&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=10))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20SCH%2023390%20and%20synthesis)]

In their published method, Elsinga et al. (8) synthesized [^11^C]verapamil by alkylation of desmethylverapamil with [^11^C]methyl iodide. After high-performance liquid chromatographic separation, radiochemical yield was 16%, based on [^11^C]methyl iodide. Total synthesis time was 45 min, and radiochemical purity was >99%. The specific activity was >11.1 TBq/mmol (300 Ci/mmol) at end of synthesis (EOS).

Wegman et al. (9) described an improved method for preparing [^11^C]verapamil by reaction of [^11^C]methyltriflate with desmethylverapamil. [^11^C]Verapamil was prepared with a reproducible radiochemical yield of 66 ± 4% (end of bombardment (EOB)) based on [^11^C]methyltriflate. Total synthesis time was 60 min. Radiochemical purity was >99%, with specific activities varying between 5 and 30 TBq/mmol (135-1110 Ci/mmol) at EOS.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Verapamil%20and%20in%20vitro)]

In the study by Elsinga et al. (8), cellular accumulation of [^11^C]verapamil was 3.5-fold higher (345 ± 102 pmol/10^6^ cells) in the human ovarian carcinoma cell line A2780 than in the corresponding Adriamycin-resistant cell line 2780AD (77 ± 15 pmol/10^6^ cells). 2780AD cells were found to have higher P-gp expression than the A2780 cells. In a study comparing a P-gp-negative small cell lung carcinoma (GLC_4_) and its overexpressing subclone (GLC_4_/P-gp), cellular accumulation of [^11^C]verapamil in GLC_4_ was 1.3-fold higher than in GLC_4_/P-gp (10). Cyclosporin A increased [^11^C]verapamil accumulation by 1.0-fold in GLC_4_/P-gp but had no effect in GLC_4_.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Verapamil%20and%20rodentia)]

Biodistribution studies in normal rats showed high accumulation of radioactivity in the lung (9.45% injected dose (ID)/g), followed by the spleen (4.54% ID/g), kidney (3.84% ID/g), pancreas (2.11% ID/g), and liver (1.35% ID/g) at 60 min after injection of [^11^C]verapamil (8). Accumulation of the tracer in the brain was low (0.14% ID/g). The heart had only moderate accumulation (0.8% ID/g). The tracer was rapidly cleared from plasma within 5 min after injection, with a first-phase half-life of 0.9 min and a second-phase half-life of 90 min. Biodistribution and PET studies in nude rats transplanted with GLC_4_ and GLC_4_/P-gp tumors showed a higher level of [^11^C]verapamil in GLC_4_ than GLC_4_/P-gp tumors (10). Pretreatment with cyclosporin A increased [^11^C]verapamil levels in GLC_4_/P-gp tumors and in the brain.

Biodistribution studies showed little difference of [^11^C]verapamil accumulation in plasma and various tissues between mdr1a(-/-) knockout mice and wild-type mice except in the brain and testes at 60 min after injection of [^11^C]verapamil (0.1 mg/kg) (11). Accumulation in the brain and testes was 8.5-fold and 2.3-fold higher in the knockout mice than the wild-type mice, which do not have the efflux pump. Cyclosporin A (50 mg/kg) increased [^11^C]verapamil accumulation in the brain (9.6-fold) and the testes (3.1-fold) in the wild-type mice, but no increases were seen in the knockout mice. This indicates that P-gp-mediated [^11^C]verapamil efflux can be modulated by cyclosporin A. About 90% of the radioactivity found in the plasma, brain, and testes of both strains of mice and in rats at 60 min after injection was intact [^11^C]verapamil. However, it was shown recently that only 27% and 48%, respectively, of the radioactivity found in the plasma and brain of rats (12) was intact [^11^C]verapamil. The main metabolites were polar and accounted for 69% (plasma) and 53% (brain) of radioactivity. These polar [^11^C]metabolites were CO_2_, urea, formaldehyde, and formaldehyde metabolites. The metabolic profile of [^11^C]verapamil in the human brain has not been identified, and it may be different from that in the rat brain. It has been postulated that most of the polar metabolites are formed in the rat brain after the parent compound crosses the BBB. This notion was supported by PET studies revealing that [^11^C]verapamil accumulation in the brain of wild-type mice was increased by cyclosporin A to levels comparable to those in the knockout mice (11) and that the influx rate constant of [^11^C]verapamil is not perfusion-dependent (11). Therefore, these metabolites should not provide a major contribution to brain concentration measurements with PET, and the increases in radioactivity may mainly reflect cyclosporin A-induced changes in P-gp-mediated efflux of [^11^C]verapamil.

Bart et al. (13) reported quantitative analysis of [^11^C]verapamil accumulation, based on distribution volume (DV, computed by Logan method using the time-activity curves in plasma and brain) in rat brains, as measured with PET. The DV in control rats was 0.65 after injection of [^11^C]verapamil (0.1 mg/kg). After modulation with 10, 15, 25, 35, and 35 mg/kg cyclosporin A, DV values increased to 0.82, 1.04, 2.85, 2.91, and 3.77, respectively. Cyclosporin A had no effect on the plasma clearance kinetics of [^11^C]verapamil and [^15^O]H_2_O brain perfusion (11). Therefore, the increases of DV may mainly reflect cyclosporin A-induced changes in P-gp-mediated efflux of [^11^C]verapamil.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Verapamil%20and%20%28pig%20or%20dog%20or%20rabbit%20or%20sheep%29)]

No relevant publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Verapamil%20and%20%28primate%20not%20human%29)]

Using PET, Lee et al. (14) obtained serial brain scans in 3 monkeys after injection of [^11^C]verapamil (65.8 ± 11.5 MBq/kg (1.8 ± 0.3 mCi/kg)) and PSC 833 (20 mg/kg/2 h). Accumulation of radioactivity (0.141 ml/g/min) was low in the brain. PSC 833 increased the accumulation significantly to 0.651 ml/g/min (P < 0.05). The accumulation of radioactivity in the cerebrum peaked at 0.58 min and remained almost constant at this level up to 60 min. About 50% of the radioactivity found in the plasma at 30 min was intact [^11^C]verapamil. PSC 833 slightly decreased the intact fraction.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Verapamil%20and%20human)]

Hendrikse et al. (15) reported on PET studies in 5 cancer patients after injection of 370 MBq (10 mCi) of [^11^C]verapamil. Accumulation of radioactivity was 43.0%, 1.3%, and 0.9% ID in the lungs, heart, and tumor, respectively. From the time-activity curves, the pharmacokinetic half-life of [^11^C]verapamil was 46.2, 73.8, and 23.7 min in the lungs, heart, and tumor, respectively. The efflux of [^11^C]verapamil out of tumors was relatively fast.

In one published study, [^11^C]verapamil (7.4 MBq/kg (0.2 mCi/kg; 0.12 μg/kg)) was administered to 12 healthy volunteers as an intravenous infusion over a period of approximately 1 min before and after at least a 1-h infusion of cyclosporin A (2.5 mg/kg/h; 2.8 ± 0.4 μmol/L) (16). Arterial blood samples and brain PET images were obtained at frequent intervals for 45 min. The brain accumulation of radioactivity (brain area under the curve/blood area under the curve) was determined in the presence and absence of cyclosporin A. The accumulation of radioactivity was increased by 88 ± 20% (1.02 ± 0.18 versus 0.55 ± 0.10; P < 0.001) in the presence of cyclosporin A without any apparent effect on cerebral blood flow, [^11^C]verapamil metabolism, or plasma protein binding. These results indicate that P-gp activity at the human BBB can be measured.

Kortekaas et al. (17) reported that the DV (Logan analysis) of [^11^C]verapamil in the midbrain was significantly increased (18%) in Parkinson’s disease (PD) patients (n = 5) compared with healthy controls (n = 5). The PD patients and controls had similar influx constants (K_1_), suggesting reduced P-gp-mediated efflux in the PD patients. Four PD patients were taking antiparkinsonian medication, and none of the controls was on any medication. This suggests a decrease in P-pg activity at the BBB of PD patients.

[^11^C]Verapamil PET is useful for objective monitoring of P-gp activity at the BBB [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20Verapamil%20and%20human)]. Internal dosimetry data for [^11^C]verapamil in humans are not available in the literature.

## References

1 Endicott J.A., Ling V. (1989). The biochemistry of P-glycoprotein-mediated multidrug resistance. Annu Rev Biochem.
2 Gottesman M.M., Pastan I. (1993). Biochemistry of multidrug resistance mediated by the multidrug transporter. Annu Rev Biochem.
3 Fojo A.T., Ueda K., Slamon D.J., Poplack D.G., Gottesman M.M., Pastan I. (1987). Expression of a multidrug-resistance gene in human tumors and tissues. Proc Natl Acad Sci U S A.
4 Piwnica-Worms D., Rao V.V., Kronauge J.F., Croop J.M. (1995). Characterization of multidrug resistance P-glycoprotein transport function with an organotechnetium cation. Biochemistry.
5 Hughes C.S., Vaden S.L., Manaugh C.A., Price G.S., Hudson L.C. (1998). Modulation of doxorubicin concentration by cyclosporin A in brain and testicular barrier tissues expressing P-glycoprotein in rats. J Neurooncol.
6 Mayer U., Wagenaar E., Dorobek B., Beijnen J.H., Borst P., Schinkel A.H. (1997). Full blockade of intestinal P-glycoprotein and extensive inhibition of blood-brain barrier P-glycoprotein by oral treatment of mice with PSC833. J Clin Invest.
7 Klohs W.D., Steinkampf R.W., Havlick M.J., Jackson R.C. (1986). Resistance to anthrapyrazoles and anthracyclines in multidrug-resistant P388 murine leukemia cells: reversal by calcium blockers and calmodulin antagonists. Cancer Res.
8 Elsinga P.H., Franssen E.J., Hendrikse N.H., Fluks L., Weemaes A.M., van der Graaf W.T., de Vries E.G., Visser G.M., Vaalburg W. (1996). Carbon-11-labeled daunorubicin and verapamil for probing P-glycoprotein in tumors with PET. J Nucl Med.
9 Wegman T.D., Maas B., Elsinga P.H., Vaalburg W. (2002). An improved method for the preparation of [11C]verapamil. Appl Radiat Isot.
10 Hendrikse N.H., de Vries E.G., Eriks-Fluks L., van der Graaf W.T., Hospers G.A., Willemsen A.T., Vaalburg W., Franssen E.J. (1999). A new in vivo method to study P-glycoprotein transport in tumors and the blood-brain barrier. Cancer Res.
11 Hendrikse N.H., Schinkel A.H., de Vries E.G., Fluks E., Van der Graaf W.T., Willemsen A.T., Vaalburg W., Franssen E.J. (1998). Complete in vivo reversal of P-glycoprotein pump function in the blood-brain barrier visualized with positron emission tomography. Br J Pharmacol.
12 Luurtsema G., Molthoff C.F., Schuit R.C., Windhorst A.D., Lammertsma A.A., Franssen E.J. (2005). Evaluation of (R)-[11C]verapamil as PET tracer of P-glycoprotein function in the blood-brain barrier: kinetics and metabolism in the rat. Nucl Med Biol.
13 Bart J., Willemsen A.T., Groen H.J., van der Graaf W.T., Wegman T.D., Vaalburg W., de Vries E.G., Hendrikse N.H. (2003). Quantitative assessment of P-glycoprotein function in the rat blood-brain barrier by distribution volume of [11C]verapamil measured with PET. Neuroimage.
14 Lee Y.J., Maeda J., Kusuhara H., Okauchi T., Inaji M., Nagai Y., Obayashi S., Nakao R., Suzuki K., Sugiyama Y., Suhara T. (2006). In vivo evaluation of P-glycoprotein function at the blood-brain barrier in nonhuman primates using [11C]verapamil. J Pharmacol Exp Ther.
15 Hendrikse N.H., de Vries E.G., Franssen E.J., Vaalburg W., van der Graaf W.T. (2001). In vivo measurement of [11C]verapamil kinetics in human tissues. Eur J Clin Pharmacol.
16 Sasongko L., Link J.M., Muzi M., Mankoff D.A., Yang X., Collier A.C., Shoner S.C., Unadkat J.D. (2005). Imaging P-glycoprotein transport activity at the human blood-brain barrier with positron emission tomography. Clin Pharmacol Ther.
17 Kortekaas R., Leenders K.L., van Oostrom J.C., Vaalburg W., Bart J., Willemsen A.T., Hendrikse N.H. (2005). Blood-brain barrier dysfunction in parkinsonian midbrain in vivo. Ann Neurol.